# N-[(1s)-1-[4-[[4-methoxy-2-[(4-[^11^C]methoxyphenyl)sulfonyl]-phenyl]sulfonyl]phenyl]ethyl]methanesulfonamide

Chemical name: | N-[(1s)-1-[4-[[4-methoxy-2-[(4-[^11^C]methoxyphenyl)sulfonyl]-phenyl]sulfonyl]phenyl]ethyl]methanesulfonamide
Abbreviated name: | [^11^C]Methoxy-Sch225336
Synonym:
Agent Category: | Compound
Target: | Cannabinoid
Target Category: | Cannabinoid CB2 receptor (CB2R)
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents | Structure of [^11^C]methoxy-Sch225336. Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=Cannabinoid+receptors)]

There are two known sub-types of the G-protein–coupled cannabinoid receptors, CB1R and CB2R, and they are believed to participate in many physiological processes such as neurotransmission, energy homeostasis, and the control of immune cell function (1). The CB1R are found primarily in the brain, whereas the CB2R are expressed predominantly on immune cells (2). However, the CB2R were shown recently to be expressed on brain neurons as well and were reported to have a role in the development of conditions such as drug abuse and depression (3). The modulation of CB2R expression has been reported in astrocytic tumors, atherosclerotic and amyloid plaques, and demyelination plaques observed in multiple sclerosis (4). A variety of CB2R antagonists and agonists are commercially available, and some agonists have been shown to induce apoptosis in various tumor cell types and are used to treat pain and inflammation observed during neuropathy, cancer, multiple sclerosis, etc (5). In addition, some agonists have been used for the management of depression, attention-deficit hyperactivity, and anxiety disorders (5).

A few tritiated ligands have been used to investigate the CB2R under in vitro conditions; however, due to low specific activity and a lack of receptor selectivity, these radioligands are not considered entirely suitable to study CB1R and CB2R (4). Recently, the ^35^S-labeled compound [^35^S]Sch225336 (N-[(1s)-1-[4-[[4-methoxy-2-[(4-[^35^S]methoxyphenyl)sulfonyl]-phenyl]sulfonyl] phenyl]ethyl]methanesulfonamide), with a high specific activity, was shown to specifically bind and act as a reverse agonist for the human CB2R (hCB2R) in in vitro binding studies (6). A near-infrared (NIR)–labeled dye that specifically bound to the CB2R was developed by Bai et al. for in vitro fluorescence imaging of the receptor (7). In addition, several clinical trials (http://clinicaltrials.gov/ct2/results?term=cannabinoid+receptors) approved by the United States Food and Drug Administration are in progress to evaluate the use of positron emission tomography (PET) for the imaging of CB1R. Because no suitable radiolabeled ligand is available for the noninvasive study and investigation of the CB2R, the ^11^C-labeled compound [^11^C]methoxy-Sch225336 was synthesized and evaluated by Evens et al. (4) in miceas a potential PET imaging agent.

### Other Sources of Information

Cannabinoid receptors (http://www.ncbi.nlm.nih.gov/omim?term=Cannabinoid%20receptors) in Online Mendelian Inheritance in Man (OMIM) database

Protein and mRNA (http://www.ncbi.nlm.nih.gov/nuccore/237681066?report=genbank) reference sequences of human brain CB1R (GeneID: 1268)

Protein and mRNA (http://www.ncbi.nlm.nih.gov/nuccore/NM_009924.3) reference sequences of mouse macrophage CB2R (GeneID: 12802)

Human brain CB1R (http://geneticassociationdb.nih.gov/cgi-bin/tableview.cgi?table=geneview&cond=GENE%20like%20'CNR1') in Genetic Association Database

Clinical trials (http://clinicaltrials.gov/ct2/results?term=cannabinoid+receptor+agonist) with unlabeled cannabinoid receptor agonists.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Sch225336%20synthesis&cmd=DetailsSearch)]

The synthesis and ^11^C-labeling of methoxy-Sch225336 was performed as described by Evens et al. (4). The radiochemical yield was reported to be ~35% with a purity of >99% (confirmed by co-elution with an authentic non-radioactive reference with high-performance liquid chromatography (HPLC)). The average specific activity of the labeled compound, from five labeling reactions, was 88.8 GBq/μmol (2.4 Ci/μmol) at the end of synthesis, but the total time required for the synthesis was not reported (4).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Sch225336%20in%20vitro%20studies&cmd=DetailsSearch)]

In a study to determine the partitioning coefficient of [^11^C]methoxy-Sch225336 with 1-octanol and 0.025 M phosphate buffer (pH 7.4), the log P value of the radiochemical was reported to be 2.15 (4).

In a competition binding assay using Chinese hamster ovary cells transfected with hCB1R or hCB2R with either [^3^H]-SR141716A or [^3^H]-CP55940 as radioligands, the affinity of Sch225336 was determined to be 78.5 ± 10.4 nM for hCB1R and 4.54 ± 0.48 nM for hCB2R (4). In another study using the [^35^S]-GTPγS assay, Sch225336 was shown to be a potential inverse agonist of hCB2R (see Milligan et al. (8) to read more about inverse agonists) (4).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Sch225336%20rodentia&cmd=DetailsSearch)]

Evens et al. studied the biodistribution of [^11^C]methoxy-Sch225336 in normal National Murine Research Institute mice (4). The animals (n = 4 mice per time point) were injected with the radiochemical through the tail vein, and the mice were euthanized at 2 min and 60 min postinjection (p.i.). Subsequently, the major organs and tissues were removed from the animals and weighed to determine the amount of accumulated radioactivity. Data obtained from this study were presented as percent of injected dose per gram tissue (% ID/g). Little radioactivity was found to have accumulated in most organs except the liver (51.5 ± 9.1 and 10.8 ± 1.7% ID/g at 2 min and 60 min p.i., respectively) and the intestines (12.6 ± 3.0 and 71.2 ± 6.9% ID/g at 2 min and 60 min p.i., respectively). Although a high accumulation of radioactivity (8.0 ± 1.0% ID/g) was noticed in the kidneys at 2 min p.i., the level reduced to 1.1 ± 0.3% ID/g by 60 min p.i., indicating that the radioactivity was not excreted through the urine but was cleared primarily through the hepatobiliary route. Very low amounts of label were detected in the brain at both time points (0.1 ± 0.0% ID/g both at 2 min and 60 min p.i.).

The percentage of intact [^11^C]methoxy-Sch225336 in the plasma of animals at 2, 10, and 30 min p.i. was reported to be 93, 63, and 60%, respectively as determined with reverse-phase HPLC (4). From these results the investigators concluded that the radiolabeled compound was rapidly metabolized during circulation in the animals.

From these studies, the investigators concluded that, because a very low amount of [^11^C]methoxy-Sch225336 accumulated in the mouse brain, this radioligand is useful only to investigate the peripheral tissue CB2R (e. g. spleen, Peyer’s patches and bone marrow etc.) in these animals (4). Also, because it was metabolized rapidly in the plasma, [^11^C]methoxy-Sch225336 can be used only for short durations under in vivo conditions to study the peripheral CB2R.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Sch225336%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Sch225336%20Non-Human%20Primates&cmd=DetailsSearch)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Sch225336%20Human%20Studies&cmd=DetailsSearch)]

No references are currently available.

## References

1 Graham E.S., Ashton J.C., Glass M. (2009). Cannabinoid receptors: a brief history and "what's hot". Front Biosci.
2 Takano A. (2010). The application of PET technique for the development and evaluation of novel antipsychotics. Curr Pharm Des.
3 Onaivi, E.S., H. Ishiguro, J.P. Gong, S. Patel, P.A. Meozzi, L. Myers, A. Perchuk, Z. Mora, P.A. Tagliaferro, E. Gardner, A. Brusco, B.E. Akinshola, B. Hope, J. Lujilde, T. Inada, S. Iwasaki, D. Macharia, L. Teasenfitz, T. Arinami, and G.R. Uhl, Brain neuronal CB2 cannabinoid receptors in drug abuse and depression: from mice to human subjects. PLoS One, 20083(2): p. e1640.
4 Evens N., Bosier B., Lavey B.J., Kozlowski J.A., Vermaelen P., Baudemprez L., Busson R., Lambert D.M., Van Laere K., Verbruggen A.M., Bormans G.M. (2008). Labelling and biological evaluation of [(11)C]methoxy-Sch225336: a radioligand for the cannabinoid-type 2 receptor. Nucl Med Biol.
5 Pertwee R.G. (2009). Emerging strategies for exploiting cannabinoid receptor agonists as medicines. Br J Pharmacol.
6 Gonsiorek W., Hesk D., Chen S.C., Kinsley D., Fine J.S., Jackson J.V., Bober L.A., Deno G., Bian H., Fossetta J., Lunn C.A., Kozlowski J.A., Lavey B., Piwinski J., Narula S.K., Lundell D.J., Hipkin R.W. (2006). Characterization of peripheral human cannabinoid receptor (hCB2) expression and pharmacology using a novel radioligand, [35S]Sch225336. J Biol Chem.
7 Bai M., Sexton M., Stella N., Bornhop D.J. (2008). MBC94, a conjugable ligand for cannabinoid CB 2 receptor imaging. Bioconjug Chem.
8 Milligan G. (2003). Constitutive activity and inverse agonists of G protein-coupled receptors: a current perspective. Mol Pharmacol.